# 4-[^18^F]Fluorobenzyl-triphenylphosphonium

Chemical name: | 4-[^18^F]Fluorobenzyl-triphenylphosphonium
Abbreviated name: | [^18^F]FBnTP
Synonym:
Agent Category: | Compound
Target: | Mitochondria
Target Category: | Lipophilic cation, mitochondrial membrane potential
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents; - Non-primate non-rodent mammals | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20FBnTP)]

Lipophilic cations are capable of passing through biological membranes by passive diffusion into the cytoplasm and mitochondria of cells in response to large negative plasma and mitochondrial membrane potentials. ^99m^Tc-2-Methoxyisobutylisonitrile (^99m^Tc-MIBI) and ^99m^Tc-tetrofosmin are delocalized lipophilic cations, which are rapidly taken up into cells driven by metabolic demand and membrane potential (1-4). They are used as myocardial-perfusion single-photon emission computed tomography as well as tumor imaging agents. However, the high accumulation of technetium tracers in the lung and liver may interfere with the detection of flow abnormalities in the myocardium.

Triphenylmethylphosphonium is a lipophilic cation and has been used to measure membrane potentials of cells in vitro (5). ^11^C-Labeled triphenylmethylphosphonium ([^11^C]TPMP) has been investigated as a positron emission tomography (PET) agent for myocardial and tumor imaging. [^11^C]TPMP demonstrated rapid clearance from the blood, fast accumulation and prolonged retention in the myocardium, and low lung accumulation in dogs (6). However, the short physical half-life of ^11^C (20 min) may make [^11^C]TPMP unsuitable for routine myocardial perfusion imaging in patients. Therefore, 4-[^18^F]fluorobenzyl-triphenylphosphonium ([^18^F]FBnTP) (^18^F has a physical half-life of 110 min) has been investigated as a PET agent for myocardial imaging to provide a better assessment of flow abnormalities in the myocardium. [^18^F]FBnTP may also be a tool for detection of physiological and pathological processes associated with mitochondrial dysfunction.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20FBnTP%20and%20synthesis)]

[^18^F]FBnTP was prepared as described by Madar et al. (7). [^18^F]Fluoride/Kryptofix 2.2.2/K_2_CO_3_ and 4-trimethylammoniumbenzaldehyde trifluoromethanesulfonate were heated and then eluted through a reverse solid-phase extraction cartridge and a column containing sodium borohydride and potassium carbonate. This procedure yielded 4-[^18^F]-fluorobenzyl alcohol, which was reacted with triphenylphosphine dibromide to produce [^18^F]FBnTP-bromide. Average radiochemical yield (n = 20) was 6% with a total synthesis time of 82 min. Radiochemical purity was >99% with an average specific activity of 16.7 GBq/µmol (451 mCi/µmol) at the end of synthesis.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20FBnTP%20and%20in%20vitro)]

Isolated canine heart cells (i.e., myocytes) accumulated [^18^F]FBnTP rapidly, with 30% of total radioactivity at 5 min and 40% at 15 min reaching a plateau (~45%) at 30–120 min (7). Resuspension of the myocytes in isotope-free incubation medium showed that cell-bound radioactivity was 88% and 85% of control radioactivity at 60 and 120 min, respectively. Hence, [^18^F]FBnTP was mostly retained by the myocytes with slight washout.

Madar et al. (8) demonstrated that [^18^F]FBnTP and ^3^H-labeled tetraphenylphosphonium ([^3^H]TPP) exhibited similar uptake kinetics and plateau concentrations in H345 human lung carcinoma cells. Stepwise membrane depolarization induced by increasing potassium ion concentrations resulted in a linear decrease in [^18^F]FBnTP cellular uptake similar to those measured for [^3^H]TPP. Selective collapse of mitochondrial membrane potential by carbonyl cyanide m-chlorophenylhydrazone (uncoupler) and proapoptotic staurosporine (known to decrease membrane potential) caused a marked decrease (69–85%) in cellular uptake for [^18^F]FBnTP and [^3^H]TPP compared with control. [^18^F]FBnTP is a mitochondria-targeting PET radiopharmaceutical responsive to alterations in membrane potential with voltage-dependent performance similar to that of [^3^H]TPP.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20FBnTP%20and%20rodentia)]

Madar et al. (7) determined accumulation of [^18^F]FBnTP in the femur bone of CD1 mice to be 1.38% injected dose (ID) as compared with free [^18^F]fluoride (15.3% ID). The extent of defluorination of [^18^F]FBnTP was relatively low. Further biodistribution studies in CD1 mice showed that [^18^F]FBnTP accumulated mainly in the kidney (24.7% ID/g), heart (12.2% ID/g), and liver (8.1% ID/g) with low blood radioactivity (0.05% ID/g) at 60 min after injection (8). PET imaging showed that [^18^F]FBnTP accumulated mainly in the kidney, followed by the heart and liver, with low accumulation in the lung.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20FBnTP%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

Madar et al. (7) performed quantitative PET imaging measurements of [^18^F]FBnTP binding in the heart of four mongrel dogs injected intravenously with 126–240 MBq (3.4–6.5 mCi) of [^18^F]FBnTP. PET scans showed distinct accumulation of [^18^F]FBnTP in the myocardium, which reached a plateau within 5 min and was retained up to 90 min. In contrast, the radioactivity of the blood pool in the left ventricular (LV) chamber was only 26.2% of the LV wall at 5 min and 13.4% of the LV wall at 10 min. [^18^F]FBnTP was uniformly distributed throughout the myocardium with 6–8% distribution covariance. The LV wall/blood, LV wall/lung, and LV wall/liver ratios were 16.6, 12.2, and 1.2 at 60 min, respectively. [^18^F]FBnTP whole-body distribution showed the highest accumulation in the kidney cortex, followed by the gall bladder, LV wall, and liver. Low accumulation was observed in the bone, spleen, and lung. The fraction of unchanged [^18^F]FBnTP in plasma samples as determined by high-performance liquid chromatography was 95% at 5 min and 75% at 30 min after injection.

Madar et al. (9) performed dynamic PET imaging and ex vivo biodistribution studies of [^18^F]FBnTP myocardial uptake in dogs (n = 17) with various degrees of stenosis of the left anterior descending or circumflex coronary arteries during adenosine vasodilation. The quantitative assessment of the perfusion defect was significantly (P < 0.03) more accurate with [^18^F]FBnTP than with ^99m^Tc-tetrofosmin in mild and severe stenosis compared with microsphere flow assessments. The ischemic/nonischemic (IS/NIS) ratio of both tracers correlated linearly with microsphere flow disparity with a similar slope. Flow defect contrast was 2.7 times greater for [^18^F]FBnTP than for ^99m^Tc-tetrofosmin. The [^18^F]FBnTP PET IS/NIS ratio (mild, 0.70 ± 0.04; severe, 0.46 ± 0.02) did not differ significantly (P > 0.33) from that measured ex vivo.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20FBnTP%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20FBnTP%20and%20human)]

No publication is currently available.

## NIH Support

U54 HL081028, R21 HL-72185, RO1 HL65455, RO1 AG25017, R24 CA92871

## References

1 Chernoff D.M., Strichartz G.R., Piwnica-Worms D. (1993). Membrane potential determination in large unilamellar vesicles with hexakis(2-methoxyisobutylisonitrile)technetium(I). Biochim Biophys Acta.
2 Chiu M.L., Kronauge J.F., Piwnica-Worms D. (1990). Effect of mitochondrial and plasma membrane potentials on accumulation of hexakis (2-methoxyisobutylisonitrile) technetium(I) in cultured mouse fibroblasts. J Nucl Med.
3 Molteni S.N., Seregni E., Botti C., Martinetti A., Ferrari L., Crippa F., Bombardieri E. (1999). The breast cancer cell line MCF7 as a model of 99mTc-SestaMIBI, 99mTc-tetrofosmin and 99mTc-Medronate incorporation. Anticancer Res.
4 Younes A., Songadele J.A., Maublant J., Platts E., Pickett R., Veyre A. (1995). Mechanism of uptake of technetium-tetrofosmin. II: Uptake into isolated adult rat heart mitochondria. J Nucl Cardiol.
5 Mitchell P., Moyle J. (1969). Estimation of membrane potential and pH difference across the cristae membrane of rat liver mitochondria. Eur J Biochem.
6 Krause B.J., Szabo Z., Becker L.C., Dannals R.F., Scheffel U., Seki C., Ravert H.T., Dipaola A.F., Wagner H.N. (1994). Myocardial perfusion with [11C]methyl triphenyl phosphonium: measurements of the extraction fraction and myocardial uptake. J Nucl Biol Med.
7 Madar I., Ravert H.T., Du Y., Hilton J., Volokh L., Dannals R.F., Frost J.J., Hare J.M. (2006). Characterization of Uptake of the New PET Imaging Compound 18F-Fluorobenzyl Triphenyl Phosphonium in Dog Myocardium. J Nucl Med.
8 Madar I., Ravert H., Nelkin B., Abro M., Pomper M., Dannals R., Frost J.J. (2007). Characterization of membrane potential-dependent uptake of the novel PET tracer (18)F-fluorobenzyl triphenylphosphonium cation. Eur J Nucl Med Mol Imaging.
9 Madar I., Ravert H., Dipaula A., Du Y., Dannals R.F., Becker L. (2007). Assessment of severity of coronary artery stenosis in a canine model using the PET agent 18F-fluorobenzyl triphenyl phosphonium: comparison with 99mTc-tetrofosmin. J Nucl Med.